# NFluc-FHA2-Aktpep-CFluc

Chemical name: | NFluc-FHA2-Aktpep-CFluc
Abbreviated name: | BARNCFluc
Synonym:
Agent category: | Polypeptide
Target: | Serine/threonine kinase (Akt)
Target category: | Enzyme
Method of detection: | Optical imaging
Source of signal/contrast: | Luciferin
Activation: | Yes
Studies: | - In vitro; - Rodents | No structure is currently available in PubChem (http://pubchem.ncbi.nlm.nih.gov).

## Background

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=BAR+Fluc)]

The serine/threonine kinase (Akt), also known as protein kinase B (PKB), is an enzyme that covalently attaches ATP-phosphate groups to the serine/threonine on protein substrates to alter the activity of the targeted protein (1, 2). As the human homolog of the viral oncogene v-akt, Akt has three isoforms derived for distinct genes: Akt1/PKBα, Akt2/PKBβ, and Akt3/PKBγ (3). All Akts have an NH_2_-terminal pleckstrin homology (PH) domain with an activating phosphorylation site (Thr-308) followed by a kinase domain, and a short COOH-terminal regulatory tail with an activating phosphorylation site (Ser-473) (4). The activation of Akt is initiated with the plasma membrane recruitment of phosphatidylinositol 3-kinase (PI3K), an upstream enzyme stimulated by a variety of activated growth factor receptors such as epidermal growth factor receptor (EGFR), vascular growth factor receptor (VEGFR), basic fibroblast growth factor (bFGF), and insulin-like growth factor receptor (IGFR) to generate phospholipids (phosphatidylinositol 3,4,5-triphosphate (PIP_3_)) to regulate Akt activity (4). The activation of Akt is completed via the phosphorylation of Thr-308 and Ser-473 (i.e., in Akt1), leading to increased Akt activity toward a variety of downstream substrates, such as the family of forkhead transcription factors for inhibiting tumor proliferations, the mammalian target of rapamycin (mTOR) for modulating protein synthesis, and the Bcl-xL/Bcl-2–associated death promoter (BAD) for uncontrolled proliferation (3, 5). These substrates possess a consensus motif R-X-R-XX-ST-B (X = amino acid, B = bulky hydrophobic residue) for Akt phosphorylation (6). Because Akt acts as a signal hub in the regulation of cell survival, proliferation, and growth, the elevation in Akt activity is found to be correlated with the increased tumorigenicity (1). Thus, a variety of inhibitors targeting Akt or its up- or downstream events are currently under clinical trials (7). For example, PAI-2 (triciribine) and perifosine are potent and selective inhibitors of Akt, rapamycin is an inhibitor for downstream mTOR, and LY294002 is an inhibitor for upstream PI3K. Also, molecular imaging of Akt activity has become an important approach in monitoring Akt activity in vivo.

Firefly luciferase (Fluc) is an oxygenase extracted from Photinus pyralis and has a molecular weight of 62 kDa (8). In the presence of adenosine triphosphate (ATP) and O_2_, Fluc oxidizes the heterocyclic substrate D-luciferin to oxyluciferin and emits light in the wavelength range of 400–620 nm (9). The active site of Fluc is composed of two distinct domains, a large N-terminal domain (residue 4–436) and a small C-terminal domain (residue 440–544), which are separated by a wide cleft (8). Splitting Fluc into N- and C-terminal fragments destroys its enzymatic activity, resulting in a complete loss of bioluminescence. The enzymatic activity or bioluminescence can be restored if the N- and C-terminal fragments are in close proximity (10). This led to the development of the split reporter, a novel labeling strategy for imaging protein–protein interactions in vivo (11). In this method, reporters like Fluc are dissected into two fragments and fused to a pair of proteins (A and B) that strongly interact with each other. The enzymatic activity of Fluc can be restored via a complementation strategy. In this strategy, protein A is connected with the N-terminal fragment of Fluc, and protein B is connected with the C-terminal fragment of Fluc. Interaction between protein A and B recovers the enzymatic activity of Fluc by bringing the two fragments of Fluc closely together, which allows for recovery of bioluminescence.

NFluc-FHA2-Aktpep-CFluc (BARNCFluc) is an optical agent for imaging Akt activity in vivo (2). BARNCFluc consists of four sequentially linked components: an N-terminal Fluc (N-Fluc) fragment, a forkhead-associated (FHA) domain extracted from Rad53 protein kinase (FHA2), an Akt consensus substrate peptide (QSRPRSCTWPLPRPEPRKKK) with spacer linkers (GGSGG) at both ends (Aktpep), and a C-terminal Fluc (C-Fluc). FHA2 (65 amino acids) possesses a β-sandwich that contains two antiparallel β-sheets and a short C-terminal α-helix, and it is able to recognize phosphoproteins by binding to phospho-amino acids such as phospho-Ser and phosphor-Thr (12). The phosphorylation of the Akt consensus substrate peptide in BARNCFluc provides such a target for FHA2 (2). The binding of FHA2 to the phosphorylated Ser/Thr generates steric hindrance to the intramolecular complementation of the N-Fluc and the C-Fluc fragments, leading to a split pair of N/C-Fluc fragments and loss of its bioluminescence. The loss of bioluminescence is directly proportional to the Akt activity; that is, the inhibition of Akt corresponds to enhanced bioluminescence. Thus, BARNCFluc is suitable for monitoring Akt activity in vivo.

## Synthesis

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=( BAR +Fluc)+AND+synthesis%0D%0A)]

Zhang et al. briefly described the preparation of BARNCFluc via the complementation strategy (2). Initially, the N-part of the Fluc gene was amplified by polymerase chain reaction, using primers that produced a SalI restriction site with an adjacent Kozak consensus sequence and a NotI restriction site at the 3’ end. The FHA2 gene from the Rad53p FHA2 domain was amplified with a sense primer containing a NotI site and a reverse primer containing an XbaI site. The C-part of the Fluc gene was amplified with primers that produced a 5’ XbaI restriction site followed by the Akt substrate sequence (QSRPRSCTWPLPRPEPRKKK) with the linker GGSGG flanked at each side and an EcoRI restriction site at the 3’ end. These genes were ligated to form a construct for encoding BARNCFluc with the subdomains in the order of N-Fluc, FHA2, linker, Aktpep, linker, and C-Fluc. The gene was cloned into the mammalian expression vector pEF to produce BARNCFluc plasmids. A variety of cells were transfected with the produced BARNCFluc plasmids using Fugene as transfection agent. No further analytical data were given.

## In Vitro Studies: Testing in Cells and Tissues

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=( BAR+Fluc)+AND+%22in+vitro%22)]

Zhang et al. examined the bioluminescence activity of BARNCFluc in vitro (2). D54 human glioma cells were transiently transfected with BARNCFluc plasmids to produce D54-BARNCFluc cells. After treatment with 40 μM API-2 (a potent inhibitor specific for Akt) for 1 h, a three-fold increase in the bioluminescence activity was observed in the cells compared with its pretreatment value. This reduction of the active (phosphorylated) Akt as a result of the API-2 treatment was further confirmed with Western blot analysis. As a control, D54 cells transfected with full-length Fluc plasmids or mutant BARNCFluc plasmids appeared to have no substantial changes in their bioluminescence activity when treated with API-2. Several other tumor cell lines were also examined, including human prostate carcinoma cells (DU-145) and human head and neck squamous carcinoma cells (MUSCC-1). The DU-145-BARNCFluc cells exhibited 3.5-fold increase in bioluminescence activity after treatment with 40 μM API-2 for 1 h. The MUSCC-1-BARNCFluc cells were serum-starved overnight and treated with epidermal growth factor (EGF). The EGF treatment led to an increase in phosphor-Akt and in phosphor-EGFR, as detected with Western blot analysis. Within 10 min after treatment, a 70% decrease in bioluminescence activity was observed. The specificity of BARNCFluc was evaluated with D54-BARNCFluc cells treated with two Akt inhibitors. The treatment with rapamycin, an inhibitor specific for downstream mTOR, led to no apparent alteration in the bioluminescence activity, whereas treatment with LY294002, an inhibitor specific for upstream PI3K, produced a six-fold increase in the bioluminescence activity.

Zhang et al. then assessed the dynamics of Akt activity via BARNCFluc in vitro (2). D54-BARNCFluc cells were treated with API-2 at doses of 2, 8, 20, 40, 80, and 120 μM, and their bioluminescence activity was measured at 5, 15, 30, and 60 min after treatment. In a dose-dependent manner, the bioluminescence increased rapidly for the first 5 min before reaching a plateau. Similar results were obtained when the D54-BARNCFluc cells were treated with perifosine. The correlation between the phosphor-Akt abundance and the changes in bioluminescence activity was further confirmed with Western blot analysis. In addition, extracts for D54-BARNCFluc cells treated with API-2 were prepared, in which the BARNCFluc was immunoprecipitated using a luciferase-specific antiserum and immunoblotted with a phosphor-threonine-specific antibody. In the presence of API-2, the BARNCFluc possessed substantially less phosphothreonine.

Zhang et al. used BARNCFluc to evaluate cancer therapy in vitro (2). Two human lung cancer cell lines, HCC87 and NCI-H1975, were transfected with BARNCFluc plasmids. The produced HCC87-BARNCFluc cells and NCI-H1975-BARNCFluc cells were treated with 1 μM erlotinib, an anticancer drug. These cells responded to erlotinib differently due to the mutations in the EGFR sequence. As an erlotinib-sensitive cell line, a six-fold increase in bioluminescence activity was observed in HCC87-BARNCFluc cells, whereas the erlotinib-resistant NCI-H1975-BARNCFluc cells exhibited no change in bioluminescence activity. The decrease in phosphor-EGFR and the alteration in its Akt status, which are caused by the treatment of HCC87-BARNCFluc cells with erlotinib, were further confirmed with Western blot analysis.

## Animal Studies

### Rodents

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=( BAR +Fluc) +AND++rodentia)]

Zhang et al. used BARNCFluc to examine cancer therapy in vivo (2). D54-BARNCFluc cells were implanted in the mammary fat pads of athymic CD-1 nu/nu genotype mice. When the tumors grew to 40–60 mm^3^ in volume, the mice were treated with intraperitoneal API-2 or oral perifosine. The bioluminescence images were collected after an intraperitoneal injection of 150 mg/kg luciferin before and over 48 h after treatment. The bioluminescence activity increased rapidly in the first 2 h and peaked at 6 h, with an approximately two-fold increase with 20 mg/kg API-2 and a four-fold increase for with 40 mg/kg API-2. The duration for the increased bioluminescence activity lasted nearly 36 h for the 20-mg/kg dose and 72 h for the 40-mg/kg dose. With 30 mg/kg perifosine, the bioluminescence activity increased within 6 h of treatment and remained high for >7 d caused by its very long plasma half-life in mice. In addition, mice were euthanized 6 h after treatment with API-2 or perifosine, and tumor tissues were excised for immunohistochemical staining. Using a phospho-Akt–specific antibody, decreased phospho-Akt staining was observed in the tumor treated with API-2 and perifosine compared with the control. This result exhibited an increased bioluminescence induced by a decreased Akt activity.

### Other Non-Primate Mammals

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=%22%20SUBSTANCENAME%22%5BSubstance%20Name%5D%20AND%20%28dog%20OR%20rabbit%20OR%20pig%20OR%20sheep%29)]

No publication is currently available.

### Non-Human Primates

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=(BAR +Fluc) +AND+(primate+non+human))]

No publication is currently available.

## Human Studies

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=( BAR +Fluc) +AND+human)]

No publication is currently available.

### NIH Support

CA 85878, CA 01014, CA 83099

## References

1 Zhang L., Bhojani M.S., Ross B.D., Rehemtulla A. (2008). Molecular imaging of protein kinases. Cell Cycle.
2 Zhang L., Lee K.C., Bhojani M.S., Khan A.P., Shilman A., Holland E.C., Ross B.D., Rehemtulla A. (2007). Molecular imaging of Akt kinase activity. Nat Med.
3 Hennessy B.T., Smith D.L., Ram P.T., Lu Y., Mills G.B. (2005). Exploiting the PI3K/AKT pathway for cancer drug discovery. Nat Rev Drug Discov.
4 Kunkel M.T., Ni Q., Tsien R.Y., Zhang J., Newton A.C. (2005). Spatio-temporal dynamics of protein kinase B/Akt signaling revealed by a genetically encoded fluorescent reporter. J Biol Chem.
5 Harvey R.D., Lonial S. (2007). PI3 kinase/AKT pathway as a therapeutic target in multiple myeloma. Future Oncol.
6 Yaffe M.B., Leparc G.G., Lai J., Obata T., Volinia S., Cantley L.C. (2001). A motif-based profile scanning approach for genome-wide prediction of signaling pathways. Nat Biotechnol.
7 Yang L., Dan H.C., Sun M., Liu Q., Sun X.M., Feldman R.I., Hamilton A.D., Polokoff M., Nicosia S.V., Herlyn M., Sebti S.M., Cheng J.Q. (2004). Akt/protein kinase B signaling inhibitor-2, a selective small molecule inhibitor of Akt signaling with antitumor activity in cancer cells overexpressing Akt. Cancer Res.
8 Conti E., Franks N.P., Brick P. (1996). Crystal structure of firefly luciferase throws light on a superfamily of adenylate-forming enzymes. Structure.
9 Paulmurugan R., Gambhir S.S. (2005). Firefly luciferase enzyme fragment complementation for imaging in cells and living animals. Anal Chem.
10 Ray P., Pimenta H., Paulmurugan R., Berger F., Phelps M.E., Iyer M., Gambhir S.S. (2002). Noninvasive quantitative imaging of protein-protein interactions in living subjects. Proc Natl Acad Sci U S A.
11 Ozawa T. (2006). Designing split reporter proteins for analytical tools. Anal Chim Acta.
12 Liao H., Byeon I.J., Tsai M.D. (1999). Structure and function of a new phosphopeptide-binding domain containing the FHA2 of Rad53. J Mol Biol.